# [^166^Ho]-Loaded poly(L-lactic acid) microspheres

Chemical name: | [^166^Ho]-Loaded poly(L-lactic acid) microspheres
Abbreviated name: | [^166^Ho]-PLLA-MS
Synonym: | [^166^Ho]-PLA-MS
Agent Category: | Compound
Target: | Hepatic arterioles
Target Category: | Arterioles
Method of detection: | Multimodality imaging: Magnetic resonance imaging (MRI); single-photon emission computed tomography (SPECT); gamma planar imaging
Source of signal / contrast: | ^166^Ho
Activation: | No
Studies: | - In vitro; - Rodents; - Non-primate non-rodent mammals | Structure not available in PubChem (http://pubchem.ncbi.nlm.nih.gov/).

## Background

[PubMed (http://www.ncbi.nlm.nih.gov/pubmed?term=166Ho&cmd=DetailsSearch)]

Hepatic metastases often occur in individuals having breast, colorectal, or neuroendocrine neoplastic tumors and usually indicate a poor prognosis for the patient (1). Radiotherapy or partial hepatectomy are often used for the treatment or removal of the hepatic tumors, respectively, but only 20%–30% of patients are eligible for these procedures because large or widespread lesions may occur in the organ or the patient may not benefit from either treatment due to the disease being at an advanced stage. In addition, many patients do not respond to the chemotherapeutic drugs used for the treatment of these lesions and suffer from many side effects as a result of the nonspecific cytotoxic or cytostatic activities exhibited by these drugs (1). Radioembolization of the tumors with ^90^Y-embedded microspheres (MS) were developed as an alternative treatment for this malignancy; ^90^Y is a pure high-energy β-emitter but exhibits low tissue penetration (2). This technique involves the placement of radioactive MS into the hepatic artery of the patient through a catheter; the infused MS travel to and are lodged in the tumor arterioles (the blood supply to hepatic tumors is primarily from the hepatic artery versus the hepatic portal vein for normal liver tissue) (3). Delivery of the high-energy β radiation from the MS within the tumor then proves fatal for the tumor cells. However, although this is considered to be a safe and suitable method for the treatment of hepatic malignancies, its main drawback is that after infusion into the artery, due to the low tissue penetration of the β radiations, the biodistribution of ^90^Y-embedded MS cannot be visualized accurately with nuclear imaging (1). The United States Food and Drug Administration has approved >100 clinical trials (http://clinicaltrials.gov/ct2/results?term=microspheres) to evaluate MS (with or without radionuclides) for the treatment of various diseases including cancers.

To visualize and treat hepatic neoplastic lesions, poly(L-lactic acid) microspheres loaded with radioactive holmium-166 (half-life = 26.8 h; [^166^Ho]-PLLA-MS) were developed (2). A characteristic feature of ^166^Ho is the dual emission of β and γ particles (~94% and ~6%, respectively, of the total radioactivity), making it a suitable nuclide for radioembolization or visualization of the biodistribution of the MS with single-photon emission computed tomography (SPECT) imaging (4). In addition, ^166^Ho is highly paramagnetic and can be detected easily in the tissue with magnetic resonance imaging (MRI). Also, the ^166^Ho-loaded MS can be easily produced under Good Manufacturing Practice (http://www.fda.gov/cosmetics/guidancecomplianceregulatoryinformation/goodmanufacturingpracticegmpguidelinesinspectionchecklist/default.htm) conditions (4). The biodistribution of [^166^Ho]-PLLA-MS has been investigated in rat models (5), rabbit models (with SPECT (6) and MRI (7)), and porcine models (with SPECT in vivo and MRI ex vivo (8)). The design of a phase I clinical trial using escalating doses of ^166^Ho-PLLA-MS for the treatment of patients with liver metastases was published recently by Smits et al. (1).

## Synthesis

[PubMed (http://www.ncbi.nlm.nih.gov/pubmed?term=166Ho-PLLA-MS%20synthesis&cmd=DetailsSearch)]

The synthesis of [^166^Ho]-PLLA-MS was described by Nijsen et al. (2). Characterization of the MS was performed with scanning electron microscopy, laser particle size analysis, and γ-spectrometry. The particles were reported to incorporate ~17.0 ± 0.6% ^166^Ho (w/w; n = 5) and were 20–50 μm in diameter. To obtain the best yield of the radiochemical the investigators concluded that non-radioactive [^165^Ho]-PLLA-MS should be free of water and that the high neutron flux and irradiation time of the MS should be < 1 h. The specific activity of [^166^Ho]-PLLA-MS was reported to be 75 MBq/mol (2.025 Ci/mol).

## In Vitro Studies: Testing in Cells and Tissues

[PubMed (http://www.ncbi.nlm.nih.gov/pubmed?term=166Ho-PLLA-MS%20in%20vitro&cmd=DetailsSearch)]

On incubation of the [^166^Ho]-PLLA-MS in phosphate-buffered saline (PBS; pH not reported) or pig liver homogenate at 37°C for 288 h, some morphological changes were visible in the labeled MS (2). However, the MS retained >98.0% of ^166^Ho even after 192 h incubation in PBS, plasma, leukocytes, and liver homogenate under these conditions.

Almost no degradation of the [^166^Ho]-PLLA-MS was observed when exposed to human serum for >380 h, and the spheres retained >97% of the radioactivity during this time (6).

Mumpher et al. detected [^166^Ho]-PLLA-MS in hematoxylin-eosin–stained rabbit liver sections 1 h after administration of the tracer (6). The MS were shown to have accumulated mainly in the arteries and arterioles of the organ.

Nijsen et al. showed that MRI can be used to track the movement of [^166^Ho]-PLLA-MS in rabbit livers ex vivo (7). This study showed that the MS initially accumulated in the small blood vessels of the liver and thereafter in the larger blood vessels of the liver.

## Animal Studies

### Rodents

[PubMed (http://www.ncbi.nlm.nih.gov/entrez/query.fcgi?cmd=PureSearch&db=pubmed&details_term=%22SUBSTANCENAME%22%5BSubstance%20Name%5D%20AND%20rodentia)]

The biodistribution of [^166^Ho]-PLLA-MS was investigated in rats implanted with medullary thyroid carcinoma tumors in the liver (5). The tumor-bearing animals were injected with the labeled MS with (n = 9 animals) or without (n = 6 animals) adrenaline treatment as described (5). Adrenaline is well known to increase blood flow in the liver. Control animals (n = 6 rats) had a sham implantation and were injected with the labeled MS in a similar manner. The animals were subjected to whole-body SPECT imaging using a gamma camera at 30 min and 1 day after administration of the tracer. The animals were subsequently euthanized for removal of the tumors and the major organs to determine the amount of radioactivity incorporated in the tissue. All data were presented as percent of injected dose per gram tissue (% ID/g). No significant difference in the incorporation of radioactivity was observed between animals with or without the adrenaline treatment. Approximately 37.5 ± 22.5% ID/g tracer was observed to have accumulated in the hepatic tumors of the test animals compared to ~5.0 ± 3.5% ID/g at the sham implantation site for the control animals. In general, the incorporation of radioactivity in the major organ tissues in both the experimental and the control animals ranged from <0.1% ID/g to 0.4% ID/g. A significantly (P < 0.001) higher tumor/non-tumor (T/N) tissue ratio (6.1 ± 2.9) was determined in the tumor-bearing rats compared to a T/N tissue ratio of 0.7 ± 0.5 in the sham-implanted controls. The radioactivity was confined primarily in the tumor and in the liver lobe with the implanted tumor in the tumor-bearing rats. Consequently, the T/N ratio of tumor was significantly (P = 0.003) reduced to 4.0 ± 1.6 if only the tumor-implanted lobe of the liver was taken as the non-target region to derive the ratio instead of the whole liver.

Whole-body gamma planar imaging showed that >95% of the tracer accumulated in the tumor and the liver, and there was almost no redistribution of radioactivity over time.

### Other Non-Primate Mammals

[PubMed (http://www.ncbi.nlm.nih.gov/pubmed?term=166Ho-PLLA-MS%20other%20non-primate%20mammals&cmd=DetailsSearch)]

To study the biodistribution and in vivo stability of [^166^Ho]-PLLA-MS, six anesthetized healthy New Zealand rabbits were injected with the labeled MS through the hepatic portal vein (6). Scintigraphic images acquired every 24 h from the animals showed that the liver outlines were uniformly defined and that there was negligible leaching of radioactivity from the organ. At 144 h after administration, 92.1 ± 4.7% ID/g of the tracer had accumulated in the liver followed by kidneys (1.2 ± 0.7% ID/g) and the femur (0.8 ± 0.5% ID/g). All other major organs had an accumulation of <0.2% ID/g.

In another study, four rabbits with tumors implanted in the liver were treated with approximately 50 mg (~ 640 MBq) of [^166^Ho]-PLLA-MS and gamma planar and MRI images were subsequently acquired from these animals (7). This study demonstrated that MRI could detect the radioactive, non-radioactive, and decayed [^166^Ho]-PLLA-MS for the entire time during which the MS stayed in the body. In addition, MRI could detect accumulation of the labeled MS in and around the hepatic tumors, and this observation was confirmed with whole-body gamma planar imaging three days after injection of the labeled MS. Results from this investigation indicated that MRI could be used to image [^166^Ho]-PLLA-MS therapy under in vivo conditions (7).

A scout and a treatment dose of [^166^Ho]-PLLA-MS administered to five healthy pigs through the hepatic portal artery were shown to be accurately measured qualitatively and quantitatively with SPECT (9). In addition, MRI was shown to detect low doses of the labeled MS given to the animals. From this study, the investigators concluded that the ^166^Ho-labeled MS could be detected easily in large animals using either SPECT or MRI techniques.

### Non-Human Primates

[PubMed (http://www.ncbi.nlm.nih.gov/pubmed?term=166Ho-PLLA-MS%20non-human%20primates&cmd=DetailsSearch)]

No publications are currently available.

## Human Studies

[PubMed (http://www.ncbi.nlm.nih.gov/pubmed?term=166Ho-PLLA-MS%20human%20studies&cmd=DetailsSearch)]

No publications are currently available.

## Supplemental Information

[Disclaimers]

No information is currently available.

## References

1 Smits M.L., Nijsen J.F., van den Bosch M.A., Lam M.G., Vente M.A., Huijbregts J.E., van het Schip A.D., Elschot M., Bult W., de Jong H.W., Meulenhoff P.C., Zonnenberg B.A. (2010). Holmium-166 radioembolization for the treatment of patients with liver metastases: design of the phase I HEPAR trial. J Exp Clin Cancer Res.
2 Nijsen J.F., Zonnenberg B.A., Woittiez J.R., Rook D.W., Swildens-van Woudenberg I.A., van Rijk P.P., van het Schip A.D. (1999). Holmium-166 poly lactic acid microspheres applicable for intra-arterial radionuclide therapy of hepatic malignancies: effects of preparation and neutron activation techniques. Eur J Nucl Med.
3 Ibrahim S.M., Lewandowski R.J., Sato K.T., Gates V.L., Kulik L., Mulcahy M.F., Ryu R.K., Omary R.A., Salem R. (2008). Radioembolization for the treatment of unresectable hepatocellular carcinoma: a clinical review. World J Gastroenterol.
4 Vente M.A., Nijsen J.F., de Roos R., van Steenbergen M.J., Kaaijk C.N., Koster-Ammerlaan M.J., de Leege P.F., Hennink W.E., van Het Schip A.D., Krijger G.C. (2009). Neutron activation of holmium poly(L-lactic acid) microspheres for hepatic arterial radio-embolization: a validation study. Biomed Microdevices.
5 Nijsen F., Rook D., Brandt C., Meijer R., Dullens H., Zonnenberg B., de Klerk J., van Rijk P., Hennink W., van het Schip F. (2001). Targeting of liver tumour in rats by selective delivery of holmium-166 loaded microspheres: a biodistribution study. Eur J Nucl Med.
6 Mumper R.J., Ryo U.Y., Jay M. (1991). Neutron-activated holmium-166-poly (L-lactic acid) microspheres: a potential agent for the internal radiation therapy of hepatic tumors. J Nucl Med.
7 Nijsen J.F., Seppenwoolde J.H., Havenith T., Bos C., Bakker C.J., van het Schip A.D. (2004). Liver tumors: MR imaging of radioactive holmium microspheres--phantom and rabbit study. Radiology.
8 Vente M.A., de Wit T.C., van den Bosch M.A., Bult W., Seevinck P.R., Zonnenberg B.A., de Jong H.W., Krijger G.C., Bakker C.J., van het Schip A.D., Nijsen J.F. Holmium-166 poly(L-lactic acid) microsphere radioembolisation of the liver: technical aspects studied in a large animal model. Eur Radiol.
9 Vente M.A., de Wit T.C., van den Bosch M.A., Bult W., Seevinck P.R., Zonnenberg B.A., de Jong H.W., Krijger G.C., Bakker C.J., van het Schip A.D., Nijsen J.F. (2010). Holmium-166 poly(L-lactic acid) microsphere radioembolisation of the liver: technical aspects studied in a large animal model. Eur Radiol.